# Polyion complex micelles of poly(ethylene glycol)-b-poly(L-lysine)-gadolinium-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-dextran sulfate

Chemical name: | Polyion complex micelles of poly(ethylene glycol)-b-poly(L-lysine)-gadolinium-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-dextran sulfate
Abbreviated name: | PIC micelles
Synonym:
Agent Category: | Nanoparticles
Target: | Non-targeted
Target Category: | Non-targeted
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal / contrast: | Gd
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=polymeric%20micelle%20and%20MRI)]

The polyion complex micelle of poly(ethylene glycol) (PEG)-b-poly(L-lysine) (P(Lys))-gadolinium-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (Gd-DOTA)-dextran sulfate, abbreviated as PIC micelles, is a Gd-based macromolecular contrast agent that has been developed by Shiraishi et al. for contrast-enhanced magnetic resonance imaging (MRI) (1).

Magnetization recovery in the longitudinal direction (T1) and magnetization decay in the transverse plane (T2, T2*) form the basis of soft-tissue contrast in MRI (2). Use of Gd-based contrast agents results in a decrease of T1 and thus leads to positive contrast enhancement in MR images. However, to date, the US Food and Drug Administration-approved Gd-based agents such as Gd-diethylenetriamine pentaacetic acid (Gd-DTPA) are low-molecular-weight Gd-chelates that induce a relatively low T1 relaxivity (r_1_) because of their fast rotation. Their typical r_1_ values are in the range of 3–5 (mM·s)^-1^ (2). Macromolecular Gd-chelates have been developed to improve the r_1_, and they are often synthesized with PEG, P(Lys), poly(glutamic acid), dendrimers, liposomes, or dextrans (3, 4). The large size of these macromolecular systems results in a higher r_1_ value because of the slow tumbling of macromolecules (5, 6). In animals, these macromolecular agents exhibit a long circulation time in the bloodstream and accumulate preferentially within tumors (7). However, agents with high molecular weights may fail to be excreted from the body, and a high blood concentration could result in undesirably high background (1, 2, 6).

Shiraishi et al. synthesized two types of polymeric micelle-based MRI contrast agents through conjugation of a PEG-P(Lys) block copolymer and a Gd-DOTA chelate (1, 6). One type possesses only DOTA-substituted lysine residues, and the other possesses both DOTA-substituted and unmodified lysine residues. These agents have been designed on the basis of the concept that stable Gd-chelated block copolymers produce a high r_1_, whereas formation of complex micelles lowers the r_1_ (1, 2, 6). In blood circulation, the agent presents as polymeric micelles, and the r_1_ is suppressed to a low level. The micelle structure inhibits access of water molecules to Gd ions in the inner core of polymeric micelles. In contrast, the polymeric micelles are gradually dissociated into single-polymer chains at the tumor sites. Because water molecules can easily access the Gd ions, the accumulated single-polymer chains generate a higher r_1_. Thus the micelle agent exhibits changeable r_1_via the formation and dissociation of micelle structure. In addition, a single block copolymer with a molecular weight of <30,000 can be excreted from kidneys, thus minimizing the potential toxicity of the agents.

The PEG-P(Lys-DOTA) system developed by Shiraishi et al. has multiple units of DOTA-bound lysine moiety. A fully DOTA-substituted block copolymer forms polymeric micelles, whereas insufficient DOTA conjugation to lysine residues prevents the formation of a polymeric micelle (1, 6, 8). In other words, the micelle structures do not form in the presence of a small amount of unmodified lysine residue. The Gd ion is only partially chelated to DOTA (20% of vacant DOTA) in the block copolymer even excess amount of Gd ions was added to the block copolymer because DOTA–DOTA interactions prevent the Gd ion from freely chelating into a DOTA moiety. Gd-Chelated PEG-P(Lys-DOTA) (PEG-P(Lys-DOTA-Gd)) could maintain the polymeric micelle structure. Therefore, the formation of the polymeric micelle appears to depend on interactions among vacant DOTAs. In addition, DOTA has been selected instead of DTPA because DOTA forms a more thermodynamically stable and kinetically inert complex than DTPA. The combination of PEG-P(Lys) copolymers and DOTA gives a more facile synthesis and a more stable metal chelation. Shiraishi et al. tested two micelle-based agents: PEG-P(Lys-DOTA-Gd) and PIC (1, 6). In contrast to PEG-P(Lys-DOTA-Gd) micelles, PIC micelles are prepared from the amino groups of the lysine units and oppositely charged dextran sulfate (1). The pharmacokinetics and biodistribution of the PIC micelles can be controlled through adjustment of the ratios of dextran sulfates with different molecular weights. The PIC micelles accumulate in tumors and produce a significant enhancement on MRI. This chapter summarizes the data obtained with PIC micelles. Another chapter summarizes the data obtained with PEG-P(Lys-DOTA-Gd) micelles (http://www.ncbi.nlm.nih.gov/books/NBK5330/).

### Related Resource Links:

- Agents synthesized with polymeric materials in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=polymer+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)
- Nanoparticle agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=nanoparticles+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20804796)]

Shiraishi et al. described the synthesis of PIC micelles in detail (1). PEG-P(Lys-DOTA) was synthesized by means of polymerization of ε-(benzyloxycarbonyl)-L-lysine N-carboxyanhydride from PEG-NH_2_. The desired DOTA moiety numbers in PEG-P(Lys-DOTA) were controlled via adjustment of the DOTA-OSu/polymer ratio. Gd-Chelation was induced by mixing GdCl_3_·6H_2_O and PEG-P(Lys-DOTA) to produce PEG-P(Lys-DOTA-Gd), and PIC micelles were formed by mixing PEG-P(Lys-DOTA-Gd) with a mixture of two dextran sulfates with different molecular weights (dex500k, 500 kDa; dex8k, 8 kDa). The dex500k/dex8k ratios were 1/2, 1/1, or 1/0.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20804796)]

Several PEG-P(Lys-DOTA-Gd) conjugates were synthesized, and in vitro characterization showed that one of the obtained PEG-P(Lys-DOTA-Gd) conjugates had 118 ethylene glycol units (molecular weight = 5,200), 65 lysine units, 13 DOTA conjugated to lysine residues, and 10 Gd ions, which was coded as 118-65-13-10. The other three PEG-P(Lys-DOTA-Gd) conjugates were similarly coded as 118-23-9-7, 118-23-23-7, and 272-22-10-8 (1).

The r_1_ values of all PEG-P(Lys-DOTA-Gd) conjugates were measured at 9.4 T (1). All of the obtained block copolymers exhibited a larger r_1_ value than that exhibited by Gd-DTPA. The r_1_ values ((mM·s)^-1^) were 3.7 for Gd-DTPA, 5.6 for 118-23-9-7, 6.1 for 118-65-13-10, 6.2 for 118-23-23-7, and 7.3 for 272-22-10-8. These results indicated that, to a certain extent, the chain length of PEG affected the r_1_ value.

The PIC micelles, produced by mixing various ratios of dex500k and dex8k, exhibited a diameter of 80–110 nm in cumulative size, near zero or slightly negative ζ-potentials, and 20%–30% decreases in r_1_ (4.4–4.7) (1).

In vitro MRI showed that 118-65-13-10 copolymers (no micelle formation) produced considerably higher signal intensity than that observed with Gd-DTPA. In contrast, the PIC micelles yielded clearly darker images than the parent block copolymers, confirming that formation of the PIC micelles lowered the signal intensity on T1-weighted images (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20804796)]

Biodistribution studies in CDF_1_ female mice bearing colon 26 tumors (n = 3 mice/time point) showed that the distribution of PIC micelles depended on the dex500k/dex8k ratio (1). When the dex500k/dex8k ratio was 1/2 or 1/1, rapid clearance from kidneys was observed, indicating that the PIC micelles were not stable in blood for a long time. When PEG-P(Lys-DOTA-Gd) was mixed with dex500k only, higher accumulation in the liver and spleen was observed. In contrast, an equal ratio of dex500k and dex8k showed better tumor accumulation and lower accumulation in the liver and spleen. The PIC micelles had a better Gd concentration in blood over time than did Gd-DTPA as shown by studies of blood-concentration time course (n = 3 mice/time point per agent).

T_1_-Weighted gradient echo axial imaging was performed with the PIC micelles with a dex500k/dex8k ratio of 1/1 (n = 3 mice) (1). Signal enhancement (1.4 times) in the tumor area was observed at 24 h after injection of the agent.

Toxicity studies showed that, when the 118-65-13-10 block copolymer alone was intravenously injected into the mouse tail vein at a dose of 0.05 mmol Gd/kg, acute death of the injected mice (3 deaths of 3 injected mice) was observed within 120 min after injection (1). This is thought to result from the toxicity that is frequently observed for polycations. In contrast, this acute toxic death was not observed in the three mice injected with PIC micelles at the equivalent dose of Gd ions. The survival of injected mice was observed for up to 8 days without any unusual behavior. The body-weight loss was within 5%. This contrast in findings indicates that PIC micelle formation effectively reduced the toxicity. The in vivo toxicity of the cationic block copolymer was totally suppressed, at least in an acute phase, by micelle formation with a polyanion (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Shiraishi K., et al. (2010). Polyion complex micelle MRI contrast agents from poly(ethylene glycol)-b-poly(l-lysine) block copolymers having Gd-DOTA; preparations and their control of T(1)-relaxivities and blood circulation characteristics. J Control Release.
2 Makowski M.R., et al. (2009). Molecular imaging with targeted contrast agents. Top Magn Reson Imaging.
3 Torchilin V.P. (2000). Polymeric contrast agents for medical imaging. Curr Pharm Biotechnol.
4 Bae Y., Kataoka K. (2009). Intelligent polymeric micelles from functional poly(ethylene glycol)-poly(amino acid) block copolymers. Adv Drug Deliv Rev.
5 Torchilin V.P. (2002). PEG-based micelles as carriers of contrast agents for different imaging modalities. Adv Drug Deliv Rev.
6 Shiraishi K., et al. (2009). Preparation and in vivo imaging of PEG-poly(L-lysine)-based polymeric micelle MRI contrast agents. J Control Release.
7 Ma H., et al. (2010). Accelerated blood clearance was not induced for a gadolinium-containing PEG-poly(L-lysine)-based polymeric micelle in mice. Pharm Res.
8 Nakamura E., et al. (2006). A polymeric micelle MRI contrast agent with changeable relaxivity. J Control Release.